# 1-([4-methoxy-^11^C]-3,4-Dimethoxyphenethyl)-4-(3-phenylpropyl)piperazinephenoxy)

Chemical name: | 1-([4-methoxy-^11^C]-3,4-Dimethoxyphenethyl)-4-(3-phenylpropyl)piperazine
Abbreviated name: | [^11^C]SA4503
Synonym:
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA4503)]

1-([4-methoxy-^11^C]-3,4-Dimethoxyphenethyl)-4-(3-phenylpropyl)piperazine ([^11^C]SA4503) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors. [^11^C]SA4503 is a potent σ_1_ receptor agonist labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

σ receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs (2). The CNS σ receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of σ receptors: σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacologic and physiologic functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. Phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (4, 5). These receptors are also expressed on a number of human and murine tumors (6).

The σ_1_ receptor subtypes have a molecular weight of ≈25 kDa, and through the process of cloning they have shown a 30% sequence homology with the yeast C89-C7 sterol isomerase (2, 7, 8) The σ_2_ receptor subtypes have a molecular weight of ≈21.5 kDa and have not been cloned. The σ_1_ receptors are thought to be involved in certain neuropsychiatric disorders, and the σ_2_ receptors are also implicated in malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. Matsuno et al. (9) developed a potent σ_1_ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which is undergoing phase II clinical trials as a therapeutic agent for functional recovery after stroke. SA4503 is highly selective for σ_1_ receptors versus σ_2_ receptors (9). Small modifications in the SA4503 structure appear to have profound effects on the σ_1_/σ_2_ receptor affinity and selectivity (10). SA5403 can be labeled with ^11^C for PET studies of σ receptors, and studies have shown specific localization of [^11^C]SA4503 in animals and humans (1, 11, 12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29SA4503%20AND%20synthesis)]

Fujimura et al. (13) reported the synthesis of SA4503 and other analogs of lefetamine. SA4503 was obtained by reacting N,N-bis(2-chloroethyl)-2-(3m4-dimethoxy)phenylethylamine with phenylpropylamine. Kawamura et al. (1, 14) prepared [^11^C]SA4503 by methylation of the demethyl precursor, O-desmethyl SA4503, with [^11^C]methyl iodide ([^11^C]CH_3_I). [^11^C]CH_3_I was synthesized with an automated system and was trapped in N,N-dimethylformamide (DMF) that contained sodium hydride (NaH) which was preheated at 80 ºC for 2-5 min before reaction. The mixture was then heated at 120 ºC for 1 min. The final product was purified by high- performance liquid chromatography (HPLC). The synthesis time was 20 min with a radiochemical purity >98%. The decay-corrected radiochemical yield was 25% (based on [^11^C]CH_3_I), and the specific activity was 46 TBq/mmol(1,242 Ci/mmol) 20 min after the end of bombardment.

[^11^C]methyl triflate ([^11^C]CH_3_Tf) was used by Kawamura and Ishiwata (15) to improve the radiosynthesis of [^11^C]SA4503. The precursor, 4-O-demethyl SA4503, was prepared from 3-phenyl-1-propanol (16). [^11^C]CH_3_Tf) was prepared by passing [^11^C]CH_3_I through silver triflate at 200 ºC with a nitrogen flow. [^11^C]CH_3_Tf was trapped in DMF that contained 4-O-demethyl SA4503 at −17 to −12ºC, and then the mixture was heated for 1 min at 120ºC. The reaction mixture was separated by HPLC. The radiochemical yield of [^11^C]SA4503 was increased to 56.2 ± 2.3%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B11C%5DSA4503%20AND%20in%20vitro)]

Kawamura et al. (16) reported that the lipophilicity logP_7.4_ (n-octanol and phosphate buffer, pH 7.4 at 37ºC) of [^11^C]SA4503 (specific activity = 135 ± 82 TBq/mmol(3,645 ± 2,214Ci/ mmol) was 2.5, and the in vitro affinity IC_50_ values in guinea pig brain membranes were 17 and 1800 nM for σ_1_ and σ_2_ receptors, respectively. Ishiwata et al. (17) reported an age-related increase in the binding of [^11^C]SA4503 to σ receptors in the rat brain membrane binding assay studies. The K_d_ values (n = 3) were 4.5 ± 0.1, 9.5 ± 0.6, 5.8 ± 0.6, and16.9 ± 0.9 nM for rats of 1.5, 6, 12, and 24 months of age, respectively. The B_max_ values were 234 ± 4, 421± 24, 545 ± 41, and 1069 ± 56 fmol/mg, respectively.

Kawamura et al. (11) studied the effects of SA4503 on proliferation of AH109A hepatoma cells (810 fmol/mg σ_1_ and 1,200 fmol/mg σ_2_), and found that SA4503 showed little tendency toward tumor growth inhibition. Van Waarde et al. (12) reported rapid association of [^11^C]SA4503 with rat glioma C6 and human small cell lung carcinoma N417 cell lines. In vitro cell binding assays indicated that the binding occurred at a single site with IC_50_ values in the 10−^5^ to 10−^4^ mol/L range.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA4503%20AND%20rodentia)]

Mouse radiation dosimetry studies indicated that the liver received the highest radiation dose of 20.5 μGy/MBq (75.9 mrad/mCi) (18). The pancreas, kidneys, lungs, and bones received 19.9 μGy/MBq ( 73.7 mrad/mCi), 19.1 μGy/MBq (70.7 mrad/mCi), 4.19 μGy/MBq (15.5 mrad/mCi), and 17.1 μGy/MBq ( 63.3 mrad/mCi), respectively. In tissue distribution studies of [^11^C]SA4503 at dosage levels of 1−2 MBq/8.2−34 pmol (27−54 μCi)/8.2−34 pmol) in mice showed radioactivity levels (n = 4) of 3.61 ± 0.39% injected dose (ID/g) at 5 min, 3.54 ± 0.38% ID/g at 15 min, 3.36 ± 0.26% ID/g at 30 min, 3.10 ± 0.23% ID/g at 60 min, and 2.79 ± 0.35% ID/g at 90 min in the brain (16, 18). Whereas the radioactivity levels in the lungs and kidneys decreased over time, radioactivity levels in the liver and pancreas increased over time. Brain uptake was significantly decreased by co-injection of unlabeled SA4503 (60% decrease) or haloperidol (a σ_1_ and σ_2_ receptor ligand). Metabolite analysis showed that 97 ± 0.9% and 54 ± 5.8% of [^11^C]SA4503 remained unchanged at 30 min after injection into the brain and plasma, respectively. Kawamura et al. (19) found that the mouse brain uptake of [^11^C]SA4503 radioactivity was not affected by cyclosporine A, a P-glycoprotein modulator. Ishiwata et al. (20) also reported that raclopride (dopamine D_2_-receptor ligand) had no effect on [^11^C]SA4503 radioactivity uptake in the mouse brain.

Ex vivo autoradiography in rat brains (98−180 MBq/2.1−7.6 nmol [2.6-4.9 mCi/2.1−7.6 nmol]) at 30 min after injection showed a higher density in the vestibular nucleus, temporal cortex, cingulated cortex, inferior colliculus, thalamus, and frontal cortex (16). Moderate levels were found in the caudate putamen and parietal cortex. In a separate study, unlabeled SA4503 reduced 80% of the density in the regions with high and moderate levels (1). Kawamura et al. (1) reported the tissue distribution study of 10 mBq/140 pmol (270 μCi/140 pmol, 0.54 nmol/kg) of [^11^C]SA4503 in rats. At 30 min after injection, the radioactivity levels (n = 4) were 0.30 ± 0.02% ID (brain), 3.84 ± 0.29% ID(pancreas), 1.40 ± 0.09% ID(liver), 1.05 ± 0.12% ID(lung), and 0.86 ± 0.04% ID(kidney), 0.98 ± 0.09% ID(spleen). The brain activity was reduced to ≈30% of the control by unlabeled SA4503 or haloperidol. In PET imaging of the rat brain 9.4 MBq/230 pmol [254 μCi/230 pmol], 0.91 nmol/kg), the rat brain was clearly visualized.

In a distribution study of 20 MBq (0.54 mCi) [^11^C]SA4503 in nude rats with C6 glioma the standardized uptake value (SUV = cpm/g tissue divided by cpm/g of body weight) was 0.65 ± 0.15 (n = 5 ) for the tumor at 60 min after injection (12). The ratios of tumor/plasma and tumor/muscle were 13.3 ± 3.1 and 5.0 ± 2.5, respectively. In another study, van Waarde et al. (21) found that [^11^C]SA4503 was fairly tumor selective for tumor cells from inflammation caused by turpentine. The SUV values (n = 6) were 0.73 ± 0.32 and 0.20 ± 0.07 for C6 tumor and inflammation, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA4503%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Kawamura et al. (18) evaluated PET imaging of [^11^C]SA4503 in a cat with a dose of 200 MBq/57 nmol (5.4 mCi/57 nmol). A high radioactivity uptake was observed in the cortex. With co-injection dose of 1 mg/kg unlabeled SA 4503, the radioactivity rapidly decreased with 67%, 47%, and 41% remaining at 30 min, 60 min, and 90 min, respectively. The blood and plasma radioactivity rapidly decreased after injection. Percentages of unchanged [^11^C]SA4503 in the blood were 26.3% (15 min), 21.9% (30 min), 12.5% (60 min), and 11.0% (90 min).

In a VX-2 carcinoma rabbit model (11,000 fmol/mg σ receptor density in cells), Kawamura et al. (11) showed that PET imaging with [^11^C]SA4503 clearly visualized VX-2 tumor tissue. Pretreatment with haloperidol or unlabeled SA4503 decreased the uptake of the radioactivity at 30 min after injection by 22% and 41%, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA4503%20AND%20%28primate%20NOT%20human%29)]

Ishiwata et al. (22) performed [^11^C]SA4503 PET imaging in a conscious monkey with a dose of 600 MBq/20 nmol(16.2 mCi/20 nmol). Images were acquired at 60 min after injection for 20 min. The accumulated radioactivity levels were relatively high in the thalamus, parietal cortex, and vermis but were relatively low in the frontal cortex and cerebellar hemisphere. The plasma radioactivity was lower than the radioactivity of blood. The radioactivity in both the blood and plasma decreased for the first 30 min. When a second dose of 140 MBq/12 μmol (3.8 mCi/12 μmol) was given to the same monkey along with 5.4 mg unlabeled SA4503 (90 min after the first scan), the initial radioactivity uptake rapidly decreased and the brain accumulation disappeared. The overall radioactivity level was ≈50−60% of the level of [^11^C]SA4503 injection alone at 60−80 min. The plasma radioactivity was slightly higher than the radioactivity of blood. The radioactivity in the blood and plasma rapidly decreased for the first 5 min and then remained constant. The authors suggested there was a saturable uptake by the blood cells or a saturable binding to the membrane. In another monkey, 1 mg/kg haloperidol was given after injection of 560 MBq/22 nmol (15.1 mCi/22 nmol) [^11^C]SA4503 was injected. The radioactivity level gradually decreased in all brain regions studied. Similarly, the radioactivity level rapidly decreased when haloperidol was given before the dose of [^11^C]SA4503.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B11C%5DSA4503%20AND%20human)]

Van Waarde et al (12) performed [^11^C]SA4503 PET imaging in a healthy human volunteer. A dose of 560 MBq/9/7 nmol (15.1 mCi/9.7 nmol) with specific activity >10 TBq/mmol (270 Ci/mmol) was administered. Imaging showed that there was high uptake in the brain, heart, liver, and kidneys. There was relatively low radioactivity in the thorax, extremities, and lower abdomen.

## References

1 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
5 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
6 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
7 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.
8 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
9 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
10 Elsinga P.H., Kawamura K., Kobayashi T., Tsukada H., Senda M., Vaalburg W., Ishiwata K. (2002). Synthesis and evaluation of [18F]fluoroethyl SA4503 as a PET ligand for the sigma receptor. Synapse.
11 Kawamura K., Kubota K., Kobayashi T., Elsinga P.H., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.
12 van Waarde A., Buursma A.R., Hospers G.A., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P.H. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
13 Fujimura K., Matsumoto J., Niwa M., Kobayashi T., Kawashima Y., In Y., Ishida T. (1997). Synthesis, structure and quantitative structure-activity relationships of sigma receptor ligands, 1-[2-(3,4-dimethoxyphenyl)ethyl]-4-(3-phenylpropyl) piperazines. Bioorg Med Chem.
14 Kawamura K., Ishiwata K., Tajima H., Ishii S., Shimada Y., Matsuno K., Homma Y., Senda M. (1999). Synthesis and in vivo evaluation of [11C]SA6298 as a PET sigma1 receptor ligand. Nucl Med Biol.
15 Kawamura K., Ishiwata K. (2004). Improved synthesis of [11C]SA4503, [11C]MPDX and [11C]TMSX by use of [11C]methyl triflate. Ann Nucl Med.
16 Kawamura K., Elsinga P.H., Kobayashi T., Ishii S., Wang W.F., Matsuno K., Vaalburg W., Ishiwata K. (2003). Synthesis and evaluation of 11C- and 18F-labeled 1-[2-(4-alkoxy-3-methoxyphenyl)ethyl]-4-(3-phenylpropyl)piperazines as sigma receptor ligands for positron emission tomography studies. Nucl Med Biol.
17 Ishiwata K., Kobayashi T., Kawamura K., Matsuno K. (2003). Age-related changes of the binding of [3h]SA4503 to sigma1 receptors in the rat brain. Ann Nucl Med.
18 Kawamura K., Ishiwata K., Shimada Y., Kimura Y., Kobayashi T., Matsuno K., Homma Y., Senda M. (2000). Preclinical evaluation of [11C]SA4503: radiation dosimetry, in vivo selectivity and PET imaging of sigma1 receptors in the cat brain. Ann Nucl Med.
19 Kawamura K., Kobayashi T., Matsuno K., Ishiwata K. (2003). Different brain kinetics of two sigma 1 receptor ligands, [3H](+)-pentazocine and [11C]SA4503, by P-glycoprotein modulation. Synapse.
20 Ishiwata K., Kobayashi T., Kawamura K., Matsuno K., Senda M. (2001). [11C]Raclopride binding was reduced in vivo by sigma(1) receptor ligand SA4503 in the mouse brain, while [11C]SA4503 binding was not by raclopride. Nucl Med Biol.
21 van Waarde A., Jager P.L., Ishiwata K., Dierckx R.A., Elsinga P.H. (2006). Comparison of Sigma-Ligands and Metabolic PET Tracers for Differentiating Tumor from Inflammation. J Nucl Med.
22 Ishiwata K., Tsukada H., Kawamura K., Kimura Y., Nishiyama S., Kobayashi T., Matsuno K., Senda M. (2001). Mapping of CNS sigma(1) receptors in the conscious monkey: preliminary PET study with [(11)C]SA4503. Synapse.